# [^99m^Tc]Human telomerase reverse-transcriptase antisense mRNA oligonucleotide

Chemical name: | [^99m^Tc]Human telomerase reverse-transcriptase antisense mRNA oligonucleotide
Abbreviated name: | [^99m^Tc]MAG3-ASON
Synonym: | ASON
Agent Category: | Oligonucleotide
Target: | Human reverse-transcriptase mRNA
Target Category: | Binding to complimentary mRNA strand
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of Signal/Contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available.

## Background

[PubMed]

Telomerase is an enzyme that synthesizes telomeric DNA at the terminal end of a chromosome, and its activation is one of the mechanisms for the progression of cancer (1). Telomerase, in conjunction with the telomere-binding proteins, maintains stability of the chromosomal terminal end by replicating the DNA, but inhibition of this activity results in a shortened telomere and ultimately leads to replicative senescence or even cell death (2). The repression and close regulation of this enzyme is considered to be one of the mechanisms for tumor suppression in humans, and there is much evidence that a shortened telomere is an indication for the development of a cancer or other degenerative disease, especially in older individuals (3-6). In addition, telomerases are specifically expressed in most cancer cell types and therefore are targets for the development of many anticancer drugs (2). Also, tumors are less likely to develop resistance to anti-telomerase drugs compared to other anticancer treatments because maintenance of the telomere and immortality is crucial for tumor progression (2). Several clinical trials (http://clinicaltrials.gov/ct2/results?term=telomerase) for drugs, vaccines, and antibodies that target the telomerases as a treatment for cancer have been approved by the United States Food and Drug Administration.

Telomerase consists of the telomerase RNA (hTR), the telomerase reverse-transcriptase (hTERT), and the associated proteins (1). Although hTR is expressed without telomerase activity both in normal cells and in malignant cells, only tumor cells express hTERT. As a consequence, hTERT is the target for the development of many anticancer therapies (7), and its expression levels may have prognostic value (8). Investigators have used only indirect methods such as immunohistochemistry, reverse-transcription polymerase chain reaction (RT-PCR), fluorescence, bioluminescence, and radionuclide imaging to determine the expression levels of hTERT in various cell types with reasonable results (9, 10). This approach may not, however, yield the exact nature of the change(s) that alter the genotype and, ultimately, the cell phenotype that result in the development of a cancer. Liu et al. envisioned that antisense oligonucleotides (ASON) would be an excellent in vivo tool to determine the level of expression of a gene during the early stages of tumor development because of their high specificity for binding to nucleotides (11). The authors investigated the in vitro activity and biodistribution of ASON directed toward the hTERT gene and labeled with radioactive technetium (^99m^Tc) in mice bearing xenograft tumors.

## Synthesis

[PubMed]

The conjugation and radiolabeling of the ASON and the sense oligonucleotides (SON) used for the following studies described by Liu et al. (11). The ASON sequence was 5’-TAGAGACGTGGCTCTTGA-3’, and the SON nucleotide sequence was 5’-TCAAGAGCCACGTCTCTA-3’. Both oligonucleotides had a primary amine on the 3’ terminal phosphate group through a six-member methylene carbon spacer. For conjugation of the ASON with the N-hydroxysuccinimidyl (NHS) derivative of S-acetylmercaptoacetyltriglycine (S-acetyl NHS-MAG3), it was dissolved in N-(2-hydroxyethyl)piperazine-N’-(2-ethanesulfonic acid) (HEPES) buffer (pH 8.0), and a fresh solution of S-acetyl NHS-MAG3 in N,N-dimethylformamide was added dropwise to a final ratio of 20:1. The mixture was incubated at room temperature for 60–120 min, and the conjugated ASON was purified with chromatography on a Sephadex G25 column using sterile phosphate buffer (pH 7.2) as an eluent. The conjugated ASON was then aliquoted into vials, lyophilized, and stored at -20°C until needed. Conjugation and storage of the SON was the same as described for the ASON (11).

For labeling with radioactive ^99m^Tc, the MAG3-ASON was dissolved in ammonium acetate buffer (pH 5.2), and sodium tartrate was added to it (as a transchelator) until the pH reached 7.6 (11). Then ^99m^Tc-pertechnetate was added, and a stannous chloride solution was added immediately. The mixture was incubated for 15–30 min, and the labeled MAG3-ASON was purified with chromatography on a Sephadex G25 column with phosphate buffer (pH 7.2) as the eluent. Labeling stability of ^99m^Tc-MAG3-ASON was determined at room temperature, in saline at room temperature, and in fresh human serum at 37°C for >24 h by paper chromatography. Stability of the labeled ASON in human serum was also determined with polyacrylamide gel electrophoresis after extraction by the phenol:chloroform method, followed by overnight ethanol precipitation at -20°C (11).

Under the conditions used, the labeling efficiency of the reaction was reported to be 76 ± 5% (n = 5 labeling reactions) with a specific activity of 10.2 kBq/pmol (0.27 μCi/pmol) and a radiochemical purity of >96% after purification (11). The Rf values for the various reaction components after paper chromatography are reported in Table 1 of the publication (11). The stability of ^99m^Tc-MAG3-ASON was reported to be >93% over a 24-h period at room temperature, in normal saline, and in fresh human serum at 37°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed]

The in vitro activity of ^99m^Tc-MAG3-ASON was investigated in HepG2 cells (11). The cells were exposed to ^99m^Tc-MAG3-ASON or ASON, and the hTERT mRNA levels in these cells were determined with RT-PCR and compared with the levels in cells exposed to ^99m^Tc-MAG3-SON or 10% fetal bovine serum (FBS). A significant reduction (P < 0.05) in the hTERT mRNA was observed in cells treated with ^99m^Tc-MAG3-ASON or ASON compared with the cells exposed either to ^99m^Tc-MAG3-SON or 10% FBS. No differences were reported in the hTERT mRNA levels of cells treated with ^99m^Tc-MAG3-ASON or ASON. Similar observations were also reported for the 10% FBS-treated cells.

## Animal Studies

### Rodents

[PubMed]

The biodistribution of ^99m^Tc-MAG3-ASON and ^99m^Tc-MAG3-SON was investigated in BALB/c nu/nu mice bearing MCF-7 cell xenograft tumors (11). The animals were injected with the labeled ASON or the SON through the tail vein and killed 0.5, 1, 2, 4, and 6 h after the injection (n = 5 animals per time point for each oligonucleotide). The various organs were harvested from the animals, weighed, and counted for radioactivity. The radioactivity had a rapid clearance from blood circulation with 2.62 ± 0.167% of the injected dose/gram tissue (% ID/g) of ^99m^Tc-MAG3-ASON remaining in the blood 0.5 h after administration. This level dropped to 1.051 ± 0.121% ID/g at 2 h. The level of ^99m^Tc-MAG3-ASON (1.157 ± 0.182% ID/g) was significantly higher (P < 0.05) compared with ^99m^Tc-MAG3-SON (0.503 ± 0.051% ID/g) in the tumors after 4 h with a tumor/muscle ratio of 8.8 and a tumor/blood ratio of 2 at 6 h. Among the various organs, maximum radioactivity was noticed in the kidneys for both the radiolabeled oligonucleotides, which indicates that the radiochemicals were cleared mainly through the urinary system.

Imaging of the mice 4–8 h after administration of the labeled oligonucleotides clearly revealed tumors only in mice injected with ^99m^Tc-MAG3-ASON (11). The tumors were not visible by imaging at any time after the administration of ^99m^Tc-MAG3-SON. However, the renal route of elimination of the radiochemicals led to an accumulation of substantial radioactivity in the abdomen with both labeled nucleotides.

### Other Non-Primate Mammals

[PubMed]

No references are currently available.

### Non-Human Primates

[PubMed]

No references are currently available.

## Human Studies

[PubMed]

No references are currently available.

## Supplemental Information

[Disclaimers]

## References

1 Kelland L. (2007). Targeting the limitless replicative potential of cancer: the telomerase/telomere pathway. Clin Cancer Res.
2 Harley C.B. (2008). Telomerase and cancer therapeutics. Nat Rev Cancer.
3 Cawthon R.M., Smith K.R., O'Brien E., Sivatchenko A., Kerber R.A. (2003). Association between telomere length in blood and mortality in people aged 60 years or older. Lancet.
4 Vulliamy T., Marrone A., Szydlo R., Walne A., Mason P.J., Dokal I. (2004). Disease anticipation is associated with progressive telomere shortening in families with dyskeratosis congenita due to mutations in TERC. Nat Genet.
5 Fitzpatrick A.L., Kronmal R.A., Gardner J.P., Psaty B.M., Jenny N.S., Tracy R.P., Walston J., Kimura M., Aviv A. (2007). Leukocyte telomere length and cardiovascular disease in the cardiovascular health study. Am J Epidemiol.
6 Armanios M.Y., Chen J.J., Cogan J.D., Alder J.K., Ingersoll R.G., Markin C., Lawson W.E., Xie M., Vulto I., Phillips J.A., Lansdorp P.M., Greider C.W., Loyd J.E. (2007). Telomerase mutations in families with idiopathic pulmonary fibrosis. N Engl J Med.
7 Deng Y., Chang S. (2007). Role of telomeres and telomerase in genomic instability, senescence and cancer. Lab Invest.
8 Lee K.H., Rudolph K.L., Ju Y.J., Greenberg R.A., Cannizzaro L., Chin L., Weiler S.R., DePinho R.A. (2001). Telomere dysfunction alters the chemotherapeutic profile of transformed cells. Proc Natl Acad Sci U S A.
9 Massoud T.F., Gambhir S.S. (2003). Molecular imaging in living subjects: seeing fundamental biological processes in a new light. Genes Dev.
10 Padmanabhan P., Otero J., Ray P., Paulmurugan R., Hoffman A.R., Gambhir S.S., Biswal S., Ulaner G.A. (2006). Visualization of telomerase reverse transcriptase (hTERT) promoter activity using a trimodality fusion reporter construct. J Nucl Med.
11 Liu M., Wang R.F., Zhang C.L., Yan P., Yu M.M., Di L.J., Liu H.J., Guo F.Q. (2007). Noninvasive imaging of human telomerase reverse transcriptase (hTERT) messenger RNA with 99mTc-radiolabeled antisense probes in malignant tumors. J Nucl Med.